# 1-(Benzofuran-2-ylmethyl)-4-(4-[^11^C]methoxybenzyl)piperazine

Chemical name: | 1-(Benzofuran-2-ylmethyl)-4-(4-[^11^C]methoxybenzyl)piperazine | [image]
Abbreviated name: | [^11^C]13 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Sigma-1 (σ1) receptor | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^11^C]13

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=sigma-1%20receptors%20and%20imaging)]

1-(Benzofuran-2-ylmethyl)-4-(4-[^11^C]methoxybenzyl)piperazine, abbreviated as [^11^C]13, is a piperazine derivative synthesized by Moussa et al. for positron emission tomography (PET) of sigma-1 (σ1) receptor (1).

σ1 receptor is a protein that is widely distributed in both the central nervous system (CNS) and peripheral organs. There are at least two subtypes of σ receptors, σ1 and σ2 receptors. Although the functions of σ2 receptor are poorly understood, σ1 receptor is believed to act as a modulator of the signal transduction in neurotransmitter systems (2, 3). σ1 receptor primarily resides at the interface between the endoplasmic reticulum and mitochondria, where it modulates Ca^2+^ flux by acting as a molecular chaperone for type 3 inositol-1,4,5-triphosphate receptors. σ1 receptor can also translocate to the plasma membrane, where it regulates the voltage-dependent Ca^2+^ channels, K^+^ channels, and other membrane-bound proteins (2, 4).

More and more evidence suggests that σ1 receptor is involved in a range of CNS diseases such as affective disorders, psychosis, schizophrenia, substance abuse, Parkinson’s disease, and Alzheimer’s disease (1, 4). Studies on postmortem human brains have shown that the density of σ1 receptor decreased in patients with schizophrenia and Alzheimer’s disease (5). Discovery of specific ligands for σ1 receptor has further prompted investigations in the imaging and treatment of neuropsychiatric diseases by targeting σ1 receptor (1, 3).

Noninvasive imaging of σ1 receptor in vivo would enable better understanding of the pathogenesis of neuropsychiatric diseases as well as how the expression and function of σ1 receptors change during disease progression (2). Early in 1998, Baziard-Mouysset et al. synthesized a series of disubstituted 1,4-piperazines, flanked by a chromene ring and a benzyl group (6). Of this series, the simplest compound that contained an unsubstituted benzyl ring displayed high affinity for σ receptors (K_i_ = 3 nM) and negligible off-target activity. Substitution of the benzyl ring was generally detrimental to σ binding, with the exception of 4-chloro or 4-methoxy substitution, which improved σ receptor binding (K_i_ = 1 nM and 0.6 nM, respectively). The chromene ring was shown to have little effect on σ binding, and it was well tolerated for substitution with a large number of alternative aromatic groups (7). With the 2-benzofurylmethyl group–substituted compound as a lead compound, Moussa et al. generated a series of N-(2-benzofuranylmethyl)-N'-(alkoxybenzyl)piperazines as selective σ1 receptor ligands (1, 4, 8). Two compounds in this series, N-(2-benzofuranylmethyl)-N'-[4-(2-fluoroethoxy)benzyl]piperazine (compound 6) and N-(benzofuran-2-ylmethyl)-N'-(4'-methoxybenzyl)piperazine (compound 13), were further radiolabeled and tested for their feasibilities as imaging probes for σ1 receptors.

This chapter summarizes the data obtained with [^11^C]13.

### Related Resource Links:

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=sigma-1%20receptors) and protein (http://www.ncbi.nlm.nih.gov/protein?term=sigma-1%20receptors) sequences of sigma-1 (σ1) receptors

Sigma-1 (σ1) receptor-related compounds (http://www.ncbi.nlm.nih.gov/pcsubstance?term=sigma-1%20receptors) in PubChem

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20662542)]

Moussa et al. described the synthesis of piperazine derivatives in detail (1). Compound 13 was synthesized by treatment of N-((benzofuran-2-yl)methyl)piperazine with 4-methoxybenzyl chloride. The chemical yield was 84%. The synthesis of [^11^C]13 was achieved by the reaction of N-((benzofuran-2-yl)methyl)-N0-(40-hydroxybenzyl)piperazine with [^11^C]CH_3_I and tetra-n-butylammonium hydroxide at room temperature for 2 min, followed by heating at 80ºC for 5 min. The radioactive fraction corresponding to [^11^C]13 was collected with semipreparative reversed-phase column chromatography, evaporated under vacuum, and reconstituted in sterile saline. The overall synthesis time of [^11^C]13 was 30 min, and the radiochemical yield was 22%. Both radiochemical and chemical purities were >98%, with a specific activity of 73 GBq/μmol (1.97 Ci/µmol) at the end of synthesis. Formulation of [^11^C]13 was achieved by dilution of the radioactive fraction of the mobile phase of high-performance liquid chromatography (HPLC) with water for injection. The final preparation was free from precursors. Administration to the animal was performed within 10 min after the end of synthesis.

The lipophilicity of compound 13 was evaluated with HPLC, which gave a log D value of 3.63 (1). To ensure high uptake in the brain and to minimize non-specific binding, the optimal log D value for therapeutic CNS-active compounds is reported to be between 2 and 3.5.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20662542)]

Affinities of compound 13 for σ1 and σ2 receptors were determined with competitive displacement of [^3^H](+)-pentazocine in a rat brain homogenate preparation (to determine σ1 receptor affinity) and with competitive displacement of [^3^H]1,3-di-(2-tolyl)-guanidine in a PC12 cell preparation (a rat pheochromocytoma cell line known to overexpress σ2 receptors) (1). Compound 13 had K_i_ values of 2.7 nM and 103 nM for σ1 and σ2 receptors, respectively, indicating selectivity for σ1 over σ2. The K_i_ values of compound 13 for 5-HT_1A_, 5-HT_2B_, and D_2_ receptors were 2,192, 15, and 2,700 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20662542)]

MicroPET studies were conducted in an anaesthetized Papio hamadryas baboon to evaluate the in vivo regional distribution kinetics of [^11^C]13 after intravenous administration of 100 MBq (2.7 mCi) [^11^C]13 (1). The microPET images confirmed the ability of [^11^C]13 to penetrate the blood–brain barrier with accumulation in the baboon brain. The time-activity curve showed that [^11^C]13 reached the maximal level within 5 min after injection and remained at a plateau to the end of the PET scan (60 min after injection). Homogenous uptake of [^11^C]13 was observed in the cingulate cortex, frontal cortex, striatum, thalamus, and cerebellum, which are known to express σ receptors. Whole-body imaging at 60 min after injection also showed accumulation of [^11^C]13 in peripheral organs, especially in the liver, which is known to contain a high density of σ1 receptors.

The in vivo specificity of [^11^C]13 uptake was evaluated in a single blocking study in the same baboon (1). Pretreatment with haloperidol (1 mg/kg) 5 min before [^11^C]13 administration resulted in increased radioligand uptake within 3 min, followed by washout. The net result was an 80% reduction in radioligand uptake in all regions of the brain at the end of the imaging experiment at 60 min when compared to [^11^C]13 administration alone, indicating the in vivo specificity of [^11^C]13 for σ receptors. Haloperidol is a high-affinity ligand for both σ receptors. The images also demonstrated significant inhibition of [^11^C]13 uptake in the liver as well as accumulation of [^11^C]13 in the kidneys and bladder, indicative of metabolism and excretion of the radioligand.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Moussa I.A., et al. (2010). Design, synthesis, and structure-affinity relationships of regioisomeric N-benzyl alkyl ether piperazine derivatives as sigma-1 receptor ligands. J Med Chem.
2 Diaz J.L., et al. (2009). Selective sigma-1 (sigma1) receptor antagonists: emerging target for the treatment of neuropathic pain. Cent Nerv Syst Agents Med Chem.
3 Berardi F., et al. (2009). 1-Cyclohexylpiperazine and 3,3-dimethylpiperidine derivatives as sigma-1 (sigma1) and sigma-2 (sigma2) receptor ligands: a review. Cent Nerv Syst Agents Med Chem.
4 Moussa I.A., et al. (2011). Synthesis and in vivo evaluation of [18F]N-(2-benzofuranylmethyl)-N'-[4-(2-fluoroethoxy)benzyl]piperazine, a novel sigma1 receptor PET imaging agent. Bioorg Med Chem Lett.
5 Jansen K.L., et al. (1993). Loss of sigma binding sites in the CA1 area of the anterior hippocampus in Alzheimer's disease correlates with CA1 pyramidal cell loss. Brain Res.
6 Baziard-Mouysset G., et al. (1998). Synthesis and structure-activity relationships of novel 2-amino alkyl chromones and related derivatives as s site-selective ligands. Eur J Med Chem.
7 Younes S., et al. (2000). Synthesis and structure-activity relationships of novel arylalkyl 4-benzyl piperazine derivatives as sigma site selective ligands. Eur J Med Chem.
8 Moussa I.A., et al. (2011). Effects of linker elongation in a series of N-(2-benzofuranylmethyl)-N'-(methoxyphenylalkyl)piperazine sigma(1) receptor ligands. Bioorg Med Chem Lett.